# ^177^Lu-Labeled sodium pyrophosphate

Chemical name: | ^177^Lu-Labeled sodium pyrophosphate | [image]
Abbreviated name: | ^177^Lu-PYP | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Bone | [image]
Target Category: | Others | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^177^Lu | [image]
Activation: | No | [image]
Studies: | - Rodents | Structure of sodium pyrophosphate (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=bisphosponate+and%20imaging%20and%20bone%20pain)]

^177^Lu-Labeled sodium pyrophosphate, abbreviated as ^177^Lu-PYP, was synthesized by Abbasi for use in imaging bone metastatic tumors and controlling metastasis-induced bone pain (1).

Malignant tumors, especially advanced carcinomas of prostate, breast, and lung, often metastasize to the bone and cause severe pain (2). Management of bone pain is challenging, and localized radiation therapy is one of the effective methods for this purpose (3-5). However, bone pain recurs at the treated sites, and patients often suffer from multiple tumor metastases. In such cases, systemic therapy and imaging with radiolabeled bone-seeking agents is one therapeutic option because of the efficacy, low cost, and low toxicity of this type of treatment. Radionuclides suitable for systemic radiotherapy of bone pain include ^32^P, ^89^Sr, ^186^Re, ^188^Re, ^153^Sm, and ^177^Lu, while bisphosphonates are often the carriers that are used to deliver the radionuclides to bone tissue because of their exceptional affinity for hydroxyapatite (1, 6). The phosphonate group in these compounds serves both as a ligand for radiometals and a functional group for hydroxyapatite binding. Radiometals have also been attached through a chelator conjugated to bisphosphonates (3).

Pyrophosphate and its analogs have long been used as bone-seeking compounds for pain relief (2). These agents differ in the efficacy and duration of pain palliation, as well as anti-tumor effect, toxicity, and cost. Abbasi labeled the pyrophosphate with ^177^Lu for both imaging and pain management purposes (1). ^177^Lu has a long half-life (t_½_ = 6.71 days) and decays to stable ^177^Hf. ^177^Lu has both beta particle emissions (E_max_ = 497 keV (78.6%), 384 keV (9.1%), and 176 keV (12.2%)) for radiotherapy and gamma emissions (E_max_ = 113 keV (6.4%) and 208 keV (11%)) for imaging. Furthermore, ^177^Lu can be generated at a large scale with excellent radionuclide purity and high specific activity. Abbasi performed single-photon emission computed tomography (SPECT) imaging with ^177^Lu-PYP and demonstrated its high uptake in the skeletal tissue of a normal rabbit, suggesting that it may be useful as a bone-pain palliation agent (1).

### Related Resource Links:

Imaging agents related to bisphosphonates (http://www.ncbi.nlm.nih.gov/books/?term=bisphosphonate%20AND%20micad%5bbook%5d) in MICAD

Bisphosphonate-related clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonate&Search=Search) in ClinicalTrials.gov

Bisphosphonate compounds (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bisphosphonate) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459337)]

Abbasi produced ^177^Lu by irradiating natural lutetium foil target at a flux of ~1.0 × 10^14^ n/cm^2^ per s for 12 h (1). The total activity was calculated to be 15,257.69 MBq (412.37 mCi), and the specific activity was ~1,388.24 MBq/mg (37.52 mCi/mg) at the end of bombardment (EOB). The measured total activity was 12,099 MBq (327 mCi) at 54 h after EOB. Analysis of the gamma ray spectrum of the irradiated target revealed major γ-peaks at 72, 113, 208, 250, and 321 keV. The radionuclide purity of ^177^Lu was >99%.

Tetrasodium pyrophosphate (purity, 95.0%; molecular weight, 265.9) was commercially available. Radiolabeling was achieved by incubation of pyrophosphate with ^177^LuCl_3_ solution for several minutes at room temperature (as labeling occurs instantly). The molar ratios of sodium pyrophosphate/Lu were 552.45, 534.76, 266.66, 159.45, 60.24, 27.25, 20.83, and 10.25, respectively, and the radiochemical yields of these formulations were determined to be 99.94 ± 0.08, 99.96 ± 0.03, 99.93 ± 0.03, 99.88 ± 0.09, 99.24 ± 0.24, 45.21 ± 0.58, 39.17 ± 0.97, and 16.33 ± 0.34%, respectively. Radiochemical purity was >99%. The specific activity was ~0.49 GBq/mg (13.16 mCi/mg). There was no significant difference for the radiochemical yield at various temperatures (20, 40, 60 and 80 °C) and at different time intervals (1, 6, 18, and 24 h) after the initiation of reaction.

The charge of ^177^Lu-PYP was determined with radio-electrophoresis (0.025 M phosphate buffer, pH 6.9) (1). ^177^LuCl_3_ did not show any movement from the point of spotting, while ^177^Lu-PYP migrated 7.0 ± 0.2 cm towards the anode within 1 h under 300 V and 45 mA, indicating a negative charge of ^177^Lu-PYP.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459337)]

No data are available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22459337)]

SPECT images were obtained at 24 h after injection of ^177^Lu-PYP (~10 MBq, ~0.27 mCi) into the ear vein of a rabbit, showing significant radioactivity in the skeleton and very high uptake in the liver (1). No detailed data were provided. No indication of whether Lu salt or LuPYP localized in the bone from the imaging experiments.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Abbasi I.A. (2012). Preliminary studies on (177)Lu-labeled sodium pyrophosphate (177Lu-PYP) as a potential bone-seeking radiopharmaceutical for bone pain palliation. Nucl Med Biol.
2 Body J.J., Mancini I. (2002). Bisphosphonates for cancer patients: why, how, and when?. Support Care Cancer.
3 Pandit-Taskar N., Batraki M., Divgi C.R. (2004). Radiopharmaceutical therapy for palliation of bone pain from osseous metastases. J Nucl Med.
4 Lam M.G., de Klerk J.M., van Rijk P.P., Zonnenberg B.A. (2007). Bone seeking radiopharmaceuticals for palliation of pain in cancer patients with osseous metastases. Anticancer Agents Med Chem.
5 Hillner B.E., Ingle J.N., Chlebowski R.T., Gralow J., Yee G.C., Janjan N.A., Cauley J.A., Blumenstein B.A., Albain K.S., Lipton A., Brown S. (2003). American Society of Clinical Oncology 2003 update on the role of bisphosphonates and bone health issues in women with breast cancer. J Clin Oncol.
6 Abbasi I.A. (2011). Studies on 177Lu-labeled methylene diphosphonate as potential bone-seeking radiopharmaceutical for bone pain palliation. Nucl Med Biol.